# ^99m^Tc-Ethylenediaminediacetic acid/hydrazinonicotinamide-[DGlu^1^]minigastrin

Chemical name: | ^99m^Tc-Ethylenediaminediacetic acid/hydrazinonicotinimide-[DGlu^1^]minigastrin
Abbreviated name: | ^99m^Tc-EDDA/HYNIC-MG0
Synonym: | ^99m^Tc-Minigastrin, ^99m^Tc-[DGlu^1^]minigastrin, ^99m^Tc-MG0
Agent Category: | Peptide
Target: | Gastrin/cholecystokinin-2 (CCK-2, CCK-B) receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | ^99m^Tc-EDDA/HYNIC-MG0, a proposed structure not yet confirmed by experiments.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin)]

^99m^Tc-Ethylenediaminediacetic acid/hydrazinonicotinamide-[DGlu^1^]minigastrin (^99m^Tc-EDDA/HYNIC-MG0) is a radiolabeled peptide developed for single-photon emission computed tomography (SPECT) imaging of tumors that express the gastrin/cholecystokinin-2 (CCK-2) receptor (1). ^99m^Tc is a gamma emitter with a physical half-life (t_½_) of 6.01 h.

The gastrointestinal peptides gastrin and CCK have various regulatory functions in the brain and gastrointestinal tract (2). Gastrin and CCK have the same COOH-terminal pentapeptide amide sequence, which is the biologically active site (3). Human gastrin is a peptide composed of 34 amino acids and also is found in several C-terminal truncated forms (4). These C-terminal truncated forms include the minigastrin, which is a 13-residue peptide with the sequence of LEEEEEAYGWMDF-NH_2_. CCKs exist in a variety of biologically active molecular forms that are derived from a precursor molecule comprising 115 amino acids (5). These forms range from 4 to 58 amino acids in length and include sulphated and unsulphated CCK-8, which has the structure DYMGWMDF-NH_2_. They bind to and act through transmembrane G-protein−coupled receptors (6). Two different CCK receptor subtypes have been identified in normal tissues. CCK-1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK-2 (CCK-B, brain) receptors have high affinity for gastrin (5). They also differ in terms of molecular structure, distribution, and affinity for CCK. These receptors have also been found to be expressed or overexpressed on a multitude of tumor types (6). CCK-2 receptors have been found most frequently in medullary thyroid carcinomas, small-cell lung cancers, astrocytomas, and stromal ovarian cancers (2). CCK-1 receptors have been identified in gastroenteropancreatic tumors, meningiomas, and neuroblastomas.

Reubi and Waser (7) designed a series of radiolabeled CCK-8 peptides that showed high specificity for potential in vivo imaging of tumors expressing CCK-2 receptors. de Jong et al. (8) developed a ^111^In-labeled nonsulfated CCK-8 analog using 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) as a bifunctional chelating agent. The radioligand showed high specific internalization rates in the receptor-positive AR42J rat pancreatic tumor cells. Because of its favorable physical properties, ^99m^Tc is still the radionuclide of choice for routine clinical applications (9). HYNIC is a bifunctional coupling agent for ^99m^Tc-labeling of peptides that can achieve high specific activities without interfering with the amino acid sequence responsible for receptor binding (10-12). In this approach, ^99m^Tc is bound to the hydrazine group, and other coordination sites are occupied by one or more coligands. The choice of coligand can influence the stability and hydrophilicity of the radiolabeled peptide. Using the HYNIC labeling strategy and EDDA or tris(hydroxymethyl)-methylglycine(tricine) as the coligand, von Guggenberg et al. (1) reported success in radiolabeling the MG0 peptide (D-Glu-Glu_5_-Ala-Tyr-Gly-Trp-Met-Asp-PheNH_2_). The ^99m^Tc-EDDA/HYNIC-MG0 peptide showed high tumor uptake in nude mice bearing AR42J tumors. However, the very high kidney activity may limit its clinical applications.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20AND%20synthesis)]

von Guggenberg et al. (1) reported the radiosynthesis of ^99m^Tc-EDDA/HYNIC-MG0 by direct EDDA labeling and tricine/EDDA exchange labeling methods. Tricine, EDDA, and HYNIC-MG0 were obtained commercially. The purity of HYNIC-MG0 was >95%. In the direct radiolabeling procedure, HYNIC-MG0 was mixed and incubated with EDDA, ^99m^Tc pertechnetate (^99m^TcO_4_−), and stannous chloride for 30 min at room temperature. The mixture was then heated for 10 min in a boiling water bath. This method resulted in very low labeling yields even at elevated temperature (80ºC) for 15 min. In the tricine/EDDA exchange method, 20 μg of HYNIC-MG0 was incubated with EDDA/tricine solution (20 mg/ml tricine, 10 mg/ml EDDA, pH 6–7), 800 MBq (21.6 mCi) ^99m^TcO_4_−, and stannous chloride (1 mg/ml in nitrogen-purged 0.1-N hydrochloric acid) for 10 min in a boiling water bath. High-performance liquid chromatography (HPLC) analysis showed a single peak with labeling yields >90%. The specific activity reported to be >70 GBq/μmol (>1.89 Ci/μmol). Further purification was achieved by solid-phase extraction (SPE) with use of a C18-SEPPAK mini-cartridge.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20AND%20in%20vitro)]

The in vitro stability of SPE-purified ^99m^Tc-EDDA/HYNIC-MG0 was tested by incubating the radiolabeled peptide in phosphate buffer (pH 7.4) and fresh human plasma at 37ºC for up to 24 h (1). After 4 h of incubation, HPLC analysis showed that the amounts of intact ^99m^Tc-EDDA/HYNIC-MG0 were 99.4% and 98.9% in the phosphate buffer and plasma, respectively. At 24 h, the amounts of intact radiolabeled peptide were 94.8% and 90.9% in the phosphate buffer and plasma, respectively. When challenged with 10,000-fold molar excess of cysteine or histidine (pH 7.4), no significant degradation was observed. In vitro plasma protein binding showed ~20% binding from 1 to 6 h of incubation of 20–100 pmol peptide/ml of human plasma at 37ºC. Incubation in kidney homogenates resulted in a very rapid degradation of ^99m^Tc-EDDA/HYNIC-MG0. After 30 min of incubation, <10% intact peptide remained. Incubation in liver homogenates, the degradation was less rapid. After 120 min incubation, 32% of the radiolabeled peptide remained intact.

The binding affinity of ^99m^Tc-EDDA/HYNIC-MG0 was tested in a competition assay against ^125^I-labeled Tyr^12^ gastrin with rat pancreatic tumor AR42J cell membranes as the source of gastrin receptors (1). The inhibition concentration (IC_50_) of the unlabeled HYNIC-MG was 15.5 nM. The dissociation constant (K_d_) and B_max_ of ^99m^Tc-EDDA/HYNIC-MG0 were 10.3 nM and 647 fmol/mg protein, respectively. AR42J cell internalization studies showed that ~10.1% of the total radioactivity was internalized after 120 min incubation (1). The radioligand was rapidly internalized after binding. After 30 min of incubation, the internalized fraction of the bound activity reached a plateau at >80%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20AND%20rodentia)]

von Guggenberg et al. (1) performed biodistribution studies of ^99m^Tc-EDDA/HYNIC-MG0 in nude mice bearing s.c. AR42J tumors (0.5–1 ml in volume). The administered dose was reported to be 1 MBq/0.15–0.2 μg peptide (27 μCi/0.15–0.2 μg peptide). At 4 h, the radioligand showed a rapid clearance and high renal excretion. The radioactivity levels (n = 3) in percent injected dose per g (% ID/g) for major organs at 4 h were 8.09 ± 1.87 (tumor), 101.00 ± 3.47 (kidney), 0.21 ± 0.07 (intestine), 0.10 ± 0.01 (liver), 0.73 ± 0.17 (stomach), 0.06 ± 0.002 (blood), 0.06 ± 0.01 (lung), and 0.06 ± 0.03 (heart). The tumor/tissue ratios were 133.75 (blood), 288.65 (muscle), 37.65 (intestine), 77.06 (liver), and 0.08 (kidney). The binding specificity was confirmed when 50 μg of human minigastrin I was coinjected with ^99m^Tc-EDDA/HYNIC-MG0, and the tumor radioactivity level was reduced to 2.96 ± 0.10% ID/g. Kidney and stomach (receptor-positive organs) activity levels were also reduced to 79.14 ± 6.98% ID/g and 0.23 ± 0.04% ID/g, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20AND%20human)]

No publication is currently available.

## References

1 von Guggenberg E., Behe M., Behr T.M., Saurer M., Seppi T., Decristoforo C. (2004). 99mTc-labeling and in vitro and in vivo evaluation of HYNIC- and (Nalpha-His)acetic acid-modified [D-Glu1]-minigastrin. Bioconjug Chem.
2 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
3 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
4 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for Peptide receptor-targeted radionuclide therapy. J Nucl Med.
5 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
6 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
7 Reubi J.C., Waser B. (1996). Unexpected high incidence of cholecystokinin-B/gastrin receptors in human medullary thyroid carcinomas. Int J Cancer.
8 de Jong M., Bakker W.H., Bernard B.F., Valkema R., Kwekkeboom D.J., Reubi J.C., Srinivasan A., Schmidt M., Krenning E.P. (1999). Preclinical and initial clinical evaluation of 111In-labeled nonsulfated CCK8 analog: a peptide for CCK-B receptor-targeted scintigraphy and radionuclide therapy. J Nucl Med.
9 Aloj L., Panico M.R., Caraco C., Zannetti A., Del Vecchio S., Di Nuzzo C., Arra C., Morelli G., Tesauro D., De Luca S., Pedone C., Salvatore M. (2002). Radiolabeling approaches for cholecystokinin B receptor imaging. Biopolymers.
10 Liu S., Edwards D.S. (1999). 99mTc-Labeled Small Peptides as Diagnostic Radiopharmaceuticals. Chem Rev.
11 Decristoforo C., Melendez-Alafort L., Sosabowski J.K., Mather S.J. (2000). 99mTc-HYNIC-[Tyr3]-octreotide for imaging somatostatin-receptor-positive tumors: preclinical evaluation and comparison with 111In-octreotide. J Nucl Med.
12 Barrett J.A., Crocker A.C., Damphousse D.J., Heminway S.J., Liu S., Edwards D.S., Lazewatsky J.L., Kagan M., Mazaika T.J., Carroll T.R. (1997). Biological evaluation of thrombus imaging agents utilizing water soluble phosphines and tricine as coligands when used to label a hydrazinonicotinamide-modified cyclic glycoprotein IIb/IIIa receptor antagonist with 99mTc. Bioconjug Chem.